# [^18^F]Fluorodipalmitin-labeled liposomes

Chemical name: | [^18^F]Fluorodipalmitin-labeled liposomes
Abbreviated name: | [^18^F]FDP-liposomes
Synonym: | 3-[^18^F]fluoro-1,2-dipalmitoyl glycerol-labeled liposomes
Agent Category: | Liposome
Target: | Non-targeted
Target Category: | Blood pool retention
Method of detection: | PET
Source of signal/contrasat: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP)]

Liposomes are double-membrane lipid vesicles (1). They have been widely studied as important carriers in controlling the spatial and temporal distribution of drug molecules or other bioactive molecules for targeted therapy; for example, they have been used as universal carriers of tumor chemotherapeutic agents, as antigen carriers to stimulate immune response, as carriers of nucleic acid for gene therapy, and as carriers of antibiotics for infectious disease treatment (2). There are many studies using ^18^F-, ^99m^Tc-, ^67^Ga-, and ^111^In-labeled liposomes for nuclear imaging, which have shown that radiolabeled liposomes exhibit good accumulation characteristics in tumor, infection, and in vivo inflammation (2). However, these radionuclides were either attached with the use of chelators that were covalently bound to the lipids or encapsulated inside the liposome hydrophilic cavity. Marik et al. (3) developed liposomes by incorporation of [^18^F]fluorodipalmitin ([^18^F]FDP) into the phospholipid bilayer to minimize internalization and metabolism in cells. Therefore, the images obtained with the use of [^18^F]FDP-liposomes could be more reflective of the biodistribution of long-circulating liposomes.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+synthesis)]

[^18^F]FDP was synthesized by nucleophilic substitution of the p-toluenesulfonyl moiety of 3-tosyl-1,2-dipalmitoyl glycerol with [^18^F]F^–^ (3). [^18^F]KF/Kryptofix 2.2.2/K_2_CO_3_ and 3-tosyl-1,2-dipalmitoyl glycerol were heated in acetonitrile to 100°C for 20 min with a decay-corrected yield of 43 ± 10% (n = 12). [^18^F]FDP was purified with chromatography and exhibited a radiochemical purity of 99%, a total synthesis time of 60 min, and a specific activity >111 GBq/mmol (3 Ci/mmol). Long-circulating radiolabeled polyethylene-glycol–coated liposomes were prepared by adding a CH_2_Cl_2_ solution of [^18^F]FDP to a mixture of 1,2-dipalmitoyl-sn-glycero-3-phosphocholine, cholesterol, 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[methoxy(polyethyleneglycol)-2000] (61:30:9). After evaporation of the solvent, phosphate-buffered saline (PBS) was added to the residue and sonicated at 50°C for 10 min. The [^18^F]FDP-liposomes were purified with gel filtration with a decay-corrected yield of 70 ± 8% (n = 4). The specific activity of the [^18^F]FDP-liposomes was 884 ± 155 MBq (23.9 ± 4.2 mCi)/mg lipid content (n = 4). The total preparation time was ~60 min. The size of the [^18^F]FDP-liposomes was 45 ± 18 nm and was stable in PBS at room temperature for 24 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+and+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+rodentia)]

Marik et al. (3) compared positron emission tomography imaging of [^18^F]FDP with [^18^F]FDP-liposomes in normal rats (n = 3) for 90 min after injection. [^18^F]FDP radioactivity accumulated mainly in the liver (5.5% injected dose (ID)/cc maximum at 5 min), spleen (4.2% ID/cc maximum at 5 min), lung (2.5% ID/cc maximum at 1 min), and blood (3% ID/cc maximum at 1 min) with low kidney accumulation (1% ID/cc maximum at 1 min). No accumulation was observed in the bones and heart. Radioactivity levels in the blood and all tissues were cleared within a few minutes. On the other hand, [^18^F]FDP-liposomes remained in the blood at near-constant levels for at least 90 min, with a maximum of 2.5% ID/cc at 2 min. [^18^F]FDP-liposomes quickly reached a plateau in the liver (1% ID/cc), spleen (1% ID/cc), kidney (1% ID/cc), and lung (2% ID/cc) in 2–3 min. The carotid vessels, the blood volume in the atria and ventricles, and the brain vasculature were clearly visualized. Minimal radioactivity was detected in the urinary bladder and heart muscle. No activity was detected in the bones and gut.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDP+human)]

No publication is currently available.

## NIH Support

R01 CA103828

## References

1 Torchilin V.P. (1996). Liposomes as delivery agents for medical imaging. Mol Med Today.
2 Torchilin V.P. (2007). Targeted pharmaceutical nanocarriers for cancer therapy and imaging. Aaps J.
3 Marik J., Tartis M.S., Zhang H., Fung J.Y., Kheirolomoom A., Sutcliffe J.L., Ferrara K.W. (2007). Long-circulating liposomes radiolabeled with [18F]fluorodipalmitin ([18F]FDP). Nucl Med Biol.